# [^99m^Tc]1,4,7,10-tetraazacyclododecane-N, N’, N’’, N’’’-tetraacetic acid-Phe-Lys-histamine-succinyl-Gly-D-Tyr-Lys- histamine-succinyl-Gly-thiosemicarbazonyl-glyoxyl-cysteine

Chemical name: | [^99m^Tc]1,4,7,10-tetraazacyclododecane-N, N’, N’’, N’’’-tetraacetic acid-Phe-Lys-histamine-succinyl-Gly-D-Tyr-Lys- histamine-succinyl-Gly-thiosemicarbazonyl-glyoxyl-cysteine
Abbreviated name: | [^99m^Tc]IMP-245
Synonym:
Agent Category: | Peptide
Target: | Carcinoembryonic antigen positive tumors
Target Category: | Antibody-ligand binding
Method of detection: | Single-photon emission computed tomography (SPECT) or gamma planar imaging
Source of Signal/Contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Bispecific+antibodies)]

Radioimmunotherapy is one of the choices available for the treatment of cancer, but this technique is not entirely successful because the antibodies (Abs) used to target the cancers are not very effective against solid tumors. This is primarily because the solid tumors have a low radiosensitivity and the Abs cannot be used to deliver a very high dose of radiation (1). The radionuclides are delivered to the tumors either by directly binding the radionuclide to the Ab that is targeted to a cellular antigen or the tumor cells are first pretargeted with an Ab and then exposed to a suitable ligand that carries the radionuclide for binding to the Ab. Use of Ab bound radioactivity usually results in hematological dose-limiting toxicity because the Ab is cleared very slowly from the blood circulation (2). Some investigators envisioned retargeting the tumors with an Ab followed by an infusion of radioactivity linked to a suitable ligand that rapidly clears from the blood and binds to the Ab would perhaps alleviate the hematological toxicity observed with radiolabeled Abs. Although there are several methods available to pretarget tumors, a common approach is to use bispecific Abs (bsAbs) - these Abs are usually genetically engineered and can bind to two distinct ligands with great specificity, inconjunction with a radiolabeled small molecule such as a hapten (3). Pretargeting with bsAbs for the treatment of tumors is under evaluation in several clinical trials (http://clinicaltrials.gov/ct2/results?term=bispecific+antibodies) approved by the United States Food and Drug Administration.

Sharkey et. al. have evaluated the use of a bispecific monoclonal antibody (bsMoAb) that is divalent for the carcinoembryonic antigen (CEA) and monovalent for anti-histamine-succinyl-glycine (HSG) for the molecular imaging of metastatic human colonic carcinoma in a mouse model (4). The structure of this bsMoAb (designated as TF2) was described by Goldenberg et. al (3). Briefly, the bsMoAb consists of three F(ab) fragments. Two of the fragments were specific for human CEA and the third fragment had binding specificity for HSG. A divalent HSG peptide labeled with radioactive 99m technetium (^99m^ Tc) was used for the imaging of tumors that bound the bsMoAb. Data obtained from the pretargeting study was compared to results obtained with radioactive fluorine (^18^F) labeled fluorodeoxyglucose ([^18^F]FDG), the HSG peptide alone or an irrelevant anti-CD22 bsMoAb.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TF2+anti-CEA+bsmAb+synthesis)]

Assembly of the TF2 anti-CEA/anti-HSG bsMoAb used for pretargeting the tumors was done by using the dock-and-lock platform technology (5) as described by Goldenberg et. al. (3). Employing recombinant DNA techniques, a cysteine modified dimerization and docking domain (called DDD2) was used to link two F(ab) fragments of the humanized MoAb hMN-14 to obtain C-DDD2-Fab-hMN-14and this was designated as the “A” component (6). The DDD2 consists of amino acids (aas) 1-44 of human tumor necrosis factor receptor RIIα and was linked to the carboxy-terminal of the Fd chain through a 14 aa flexible peptide linker. A F(ab) precursor fragment of the humanized MoAb h679 that has specificity for HSG was used to generate a second, recombinant, “B” component by linking the AD2 sequence (this is a 17 aa sequence derived from the A kinase anchor protein that is optimized for selectively binding with RII and has cysteine residues both at the N and the C terminals of the peptide) to the carboxy-terminus of the Fd chain through a 15-residue flexible peptide linker to obtain h679-AD2 (7).

Details of the production, purification and analysis of the two components are given elsewhere (5). A molar excess of component A was mixed with the B component in presence of a thiol reducing agent at room temperature for 1 h (5). The thiol reducing agent was removed by hydrophobic interaction chromatography and dimethyl sulphoxide was added to the solution for the formation of disulfide bonds. The disulfide-linked structure, designated TF2, was purified to homogeneity by affinity chromatography using HSG as the ligand (8). The stability of TF2 was determined by incubating it in pooled fresh human serum at 37^o^C under 5% CO_2_ for 7 days. The TF2 was reported to retain 98% of its bispecific binding activity after 7 days as determined by Biacore analysis (5).

The HSG containing peptide (IMP 245) was synthesized with a solid-phase, Fmoc-based method using Rink amide resin (9). The peptide was purified by reverse phase high performance liquid chromatography (RP-HPLC). The peptide was formulated into a lyophilized, single vial kit containing IMP 245, tin chloride, ascorbic acid and a 6-fold excess of unlabeled indium-to-peptide for binding to diethylenetriaminepentaacetic acid used during the synthesis and that may have co-eluted with the peptide. For labeling with radioactive technetium (^99m^Tc) the vials were reconstituted with ^99m^Tc pertechnetate in saline and incubated at room temperature for 10 min and transferred to a boiling water bath for 15 min. Purity of the ^99m^Tc labeled peptide was determined by RP-HPLC and instant thin layer chromatography. To investigate the ability of the radiolabeled peptide to bind to CEA-bound bsMAb, it was mixed with a preformed mixture of CEA and the bsMAb. The specific activity of [^99m^Tc]IMP 245 was between 1500 and 1600 Ci/mmol (5.5-5.9 TBq/mmol) with a radiochemical purity of >98% (10). A 100% of the radiolabeled peptide was reported to bind to the bsMAb (4).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+IMP+245+in+vitro)]

No references are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20rodentia)]

The biodistribution of [^99m^Tc]IMP 245 was investigated in NCr nude mice implanted with human colon cancer cell line, GW-39, tumors (10). The mice were injected with the radiochemical, sacrificed 30 min and 3 h later (n=5 animals per time point), and the radioactivity associated with the various organs determined. Results from this study indicated the labeled peptide was cleared primarily through the kidneys (8.63±2.42% of injected dose/gram tissue (%ID/g) at 30 min). During the same period only a small fraction of the radioactivity was observed in the liver (0.63±0.10%ID/g), small intestine (1.19±0.70%ID/g) and the large intestines (0.25±0.05%ID/g). The investigators also studied the biodistribution of [^99m^Tc]IMP 245 in mice after pretargeting the tumors with the bsMAb (10). The mice were injected with the labeled peptide 24 h after treatment with the bsMAb and the animals were sacrificed at different time points (n=5 mice per time point), and accumulated radioactivity in the various organs was determined. A high accumulation of the radioactivity was observed in the tumors (14.2±5.27%ID/g) at 3 h compared to the other organs (kidneys, 2.68±0.50%ID/g; liver, 0.71±0.13%ID/g; blood, 2.23±0.39%ID/g) and a low uptake was noted in the gastrointestinal tract during the same period.

In another study with bsMAb targeted mice bearing GW-39 cell xenograft tumors that were injected with the IMP 245 radiotracer 24 h after treatment with the bsMAb, xenografts as small as ~0.15 g were visible within 1 h after the administration of [^99m^Tc]IMP 245 (11). During this time the tumor/blood ratios were reported to increase ≥40-fold compared to a ^99m^Tc-labeled CEA-specific F(ab”) used clinically for colorectal cancer detection. Based on these results the investigators suggested this technology could probably be used with other antibodies and imaging modalities also (11).

The tumor specificity of [^99m^Tc]IMP 245 was clearly evident from the data obtained by Rossi et. al. in a study performed on TF2 pretargeted nude mice bearing LS-174T cell xenograft tumors (5). The tumor/nontumor ratios obtained from this study are given in the table below (ratio ± standard deviation):

Organs | Time After the Administration of [ ^ 99m ^ Tc]IMP 245 (h)
Organs | 0.5 | 1 | 4 | 24
Liver | 34 ± 4 | 83 ± 10 | 116 ± 32 | 115 ± 21
Spleen | 37 ± 4 | 109 ± 21 | 170 ± 54 | 177 ± 30
Kidneys | 3 ± 0.4 | 7 ± 2 | 11 ± 2 | 14 ± 3
Lungs | 14 ± 2 | 47 ± 4 | 106 ± 26 | 162 ± 24
Blood | 13 ± 2 | 66 ± 5 | 237 ± 36 | 395 ± 26
Stomach | 63 ± 25 | 169 ± 116 | 456 ± 271 | 135 ± 91
Small intestine | 28 ± 3 | 35 ± 5 | 114 ± 47 | 125 ± 46
Large intestine | 75 ± 17 | 241 ± 31 | 22 ± 14 | 57 ± 34
Tail | 11 ± 3 | 37 ± 8 | 164 ± 135 | 293 ± 80

Sharkey et. al. investigated the retargeting approach to detect small (<0.3 mm diameter) microdessimated human colon cancer GW-39 cell colonies in the lungs of nude mice (4). The investigators reported that by retargeting with the TF2 bsMAb the tumors were detected in lungs of the mice (n=32) within 1.5 h after administration of the [^99m^Tc]IMP 245 peptide. In another set of mice that were treated with the peptide alone (n=20 animals), an irrelevant bsMAb (anti-CD22) (n=12 animals) and retargeted peptide and those treated with [^18^F]FDG (n=15 animals) did not detect the tumors. It was also reported that uptake of the labeled peptide in the lungs tumors of the TF2 pretargeted animals was nine fold higher than in lungs of the non-pretargeted mice (4). By comparison, the uptake was only 1.5 fold higher in the tumor bearing lungs with [^18^F]FDG or the labeled peptide alone. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+IMP+245+non+primate+mammals)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+IMP+245+non+human+primates)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+IMP+245+humans)]

No publications are currently available.

## Supplemental Information

[Disclaimers]

## NIH Support

NIH Grant #

## References

1 Goldenberg D.M. (2002). Targeted therapy of cancer with radiolabeled antibodies. J Nucl Med.
2 Goldenberg D.M., Chatal J.F., Barbet J., Boerman O., Sharkey R.M. (2007). Cancer Imaging and Therapy with Bispecific Antibody Pretargeting. Update Cancer Ther.
3 Goldenberg D.M., Rossi E.A., Sharkey R.M., McBride W.J., Chang C.H. (2008). Multifunctional antibodies by the Dock-and-Lock method for improved cancer imaging and therapy by pretargeting. J Nucl Med.
4 Sharkey R.M., Karacay H., Vallabhajosula S., McBride W.J., Rossi E.A., Chang C.H., Goldsmith S.J., Goldenberg D.M. (2008). Metastatic human colonic carcinoma: molecular imaging with pretargeted SPECT and PET in a mouse model. Radiology.
5 Rossi E.A., Goldenberg D.M., Cardillo T.M., McBride W.J., Sharkey R.M., Chang C.H. (2006). Stably tethered multifunctional structures of defined composition made by the dock and lock method for use in cancer targeting. Proc Natl Acad Sci U S A.
6 Sharkey R.M. Juweid M. Shevitz J. Behr T. Dunn R. Swayne L.C. Wong G.Y. Blumenthal R.D. Griffiths G.L. Siegel J.A. Evaluation of a complementarity-determining region-grafted (humanized) anti-carcinoembryonic antigen monoclonal antibody in preclinical and clinical studies Cancer Res 1995 55Suppl23 5935s 5945s 7493374
7 Rossi E.A., Sharkey R.M., McBride W., Karacay H., Zeng L., Hansen H.J., Goldenberg D.M., Chang C.H. (2003). Development of new multivalent-bispecific agents for pretargeting tumor localization and therapy. Clin Cancer Res.
8 Rossi E.A., Chang C.H., Losman M.J., Sharkey R.M., Karacay H., McBride W., Cardillo T.M., Hansen H.J., Qu Z., Horak I.D., Goldenberg D.M. (2005). Pretargeting of carcinoembryonic antigen-expressing cancers with a trivalent bispecific fusion protein produced in myeloma cells. Clin Cancer Res.
9 Karacay H., McBride W.J., Griffiths G.L., Sharkey R.M., Barbet J., Hansen H.J., Goldenberg D.M. (2000). Experimental pretargeting studies of cancer with a humanized anti-CEA x murine anti-[In-DTPA] bispecific antibody construct and a (99m)Tc-/(188)Re-labeled peptide. Bioconjug Chem.
10 Sharkey R.M., McBride W.J., Karacay H., Chang K., Griffiths G.L., Hansen H.J., Goldenberg D.M. (2003). A universal pretargeting system for cancer detection and therapy using bispecific antibody. Cancer Res.
11 Sharkey R.M., Cardillo T.M., Rossi E.A., Chang C.H., Karacay H., McBride W.J., Hansen H.J., Horak I.D., Goldenberg D.M. (2005). Signal amplification in molecular imaging by pretargeting a multivalent, bispecific antibody. Nat Med.